# ^111^In/^125^I/^99m^Tc-Labeled N-terminus tri-(histidine-glutamate) (HE)_3_-tagged and N- or C-terminus hexahistidine (H6)-tagged anti-epidermal growth factor receptor Affibody Z_HER2:342_-C

Chemical name: | ^111^In/^125^I/^99m^Tc-Labeled N-terminus tri-(histidine-glutamate) (HE)_3_-tagged and N- or C-terminus hexahistidine (H6)-tagged anti-epidermal growth factor receptor Affibody Z_HER2:342_-C
Abbreviated name: | [^111^In/^125^I/^99m^Tc]-(HE)_3_-Z_HER2:342_-C, [^111^In/^125^I/^99m^Tc]-H_6_-Z_HER2:342_-C, and [^111^In/^125^I/^99m^Tc]-Z_HER2:342_-H_6_-C
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In/^125^I/^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20affibody&cmd=DetailsSearch)]

The epidermal growth factor receptor-2 (HER2, ErbB2) modulates its activity through a tyrosine kinase signaling pathway and is involved in the development of various types of cancers such as those of the lungs, breast, head and neck, etc (1, 2). Overexpression or amplification of the HER2 gene is known to occur in a high percentage of cancer cases (e.g., ~20% of breast cancer) and predicts a poor prognosis for the patient. Invasive methods such as biopsies in conjunction with immunohistochemistry and fluorescence in situ hybridization are often employed to assess the HER2 status of the primary and metastasized neoplastic tumors; however, because of sampling bias and tumor heterogeneity, results obtained with these procedures may not be reliable (1). Because of their small size and high chemical and thermal stability, there is much interest in the use of radiolabeled Affibodies (an Affibody molecule is a chain of 58 amino acids (~7 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained by chemical synthesis or produced in bacteria with the use of recombinant DNA technology (3)) for the targeted detection and treatment of malignant tumors as discussed in detail elsewhere (3-5). A biodistribution study using ^111^In-labeled anti-epidermal growth factor receptor (EGFR) Affibody (Z_HER:1907_; the radionuclide was chelated to the Affibody through a metal chelator) with single-photon emission computed tomography (SPECT) showed that the tracer was suitable for the molecular imaging of EGFR expression in xenograft tumors in mice (6). However, a very high accumulation of radioactivity from the labeled Affibody was found in the kidneys and suggested that the tracer should not be used to detect cancerous tumors in close proximity of these organs. Ekblad et al. showed that the position of a metal chelator on the Affibody affected the in vivo stability and biodistribution of the molecule (7).

It was reported that an anti-EGFR Affibody dimer ((Z_HER2:342_)_2_) bearing a hexa-histidine tag (H_6_) on the N-terminus (H_6_-(Z_HER2:342_)_2_) can be labeled with ^99m^Tc-tricarbonyl ([^99m^Tc(CO)_3_]^+^), and the radiolabeled Affibody ([^99m^Tc(CO)_3_]^+^-H_6_-(Z_HER2:342_)_2_) can be used to visualize tumors expressing HER2 in mice (8). With this construct, a higher amount of radioactivity was observed to accumulate in the liver compared with the tumors, and the investigators concluded that, because cancers usually metastasize to the liver, [^99m^Tc(CO)_3_]^+^-H_6_-(Z_HER2:342_)_2_ was suitable only for the imaging of extrahepatic tumors. Similar observations were also made with other anti-EGFR Affibodies (9). On the basis of a hypothesis that the uptake of a labeled compound by the liver can be reduced by removing the H_6_ tag from the N-terminus of the Z_HER2:342_ Affibody or by increasing the hydrophilicity of the tag, two new tracers were constructed by Tolmachev et al. (10). In one construct, the H_6_ tag was moved from the N-terminal of the Affibody to the C-terminal (Z_HER2:342_-H_6_); in the second construct, the tag located on the N-terminal of the Affibody was made more hydrophilic by substituting it with a glutamatic acid-histidine trimer ((HE)_3_) to generate (HE)_3_-Z_HER2:342_. These constructs were subsequently labeled with [^99m^Tc(CO)_3_]^+^ to form [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, respectively. The biodistribution patterns of these radiolabeled Affibodies were studied in normal and nude mice bearing LS174T cell xenograft tumors (the LS174T is a human colorectal cancer cell line that has a low expression of HER2) and compared it with that of the parent radiolabeled Affibody ([^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_) described previously (11). Results from this study showed that the accumulation of radioactivity in the liver with the Z_HER2:342_-H_6_ and the (HE)_3_-Z_HER2:342_ constructs was almost 10-fold lower than that with H_6_-Z_HER2:342_, and there was a similar uptake of label in the tumors with all three conjugates. In addition, the tumor/liver radioactivity ratio with [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ was far superior to that observed with the other constructs.

On the basis of observations described above, it was postulated that the use of a (HE)_3_-tag in an anti-HER2 Affibody may be useful even if the C-terminus of the molecule is modified by the addition of a cysteine (C) residue for site-specific labeling of the peptide (12). To demonstrate this, three new Affibody constructs were prepared (H_6_-Z_HER2:342_-C, Z_HER2:342_-H_6_-C, and (HE)_3_-Z_HER2:342_-C) and labeled with ^111^In, ^99m^Tc, and ^125^I, respectively. The biodistribution of the various radiolabeled Affibodies ([^111^In/^125^I/^99m^Tc]-labeled (HE)_3_-Z_HER2:342_-C, [^111^In/^125^I/^99m^Tc]-labeled H_6_-Z_HER2:342_-C, and [^111^In/^125^I/^99m^Tc]-labeled Z_HER2:342_-H_6_-C) was then studied in normal mice.

### Related Resource Links

Anti-HER2 Affibody chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-HER2+affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

HER2 clinical trials (http://clinicaltrials.gov/ct2/results?term=HER2)

Other EGFR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man database)

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20affibody%20synthesis&cmd=DetailsSearch)]

The (HE)_3_-Z_HER2:342_-C Affibody was expressed in Escherichia coli and purified from the bacteria with immobilized metal affinity chromatography using a Co^2+^ affinity resin as described by Hofstrom et al. (12). The Affibody was further purified with reversed-phase high-performance liquid chromatography (RP-HPLC), and the purified preparations were analyzed with sodium dodecyl sulfate-polyacrylamide gel electrophoresis. The final preparation of the Affibody had a purity of >95% as determined with RP-HPLC.

The different Affibody types were labeled with ^111^In, ^125^I, and ^99m^Tc as described elsewhere (12). ^111^In-Labeling of each Affibody type was done with 1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid as the chelator (DOTA; [^111^In]-DOTA-(HE)_3_-Z_HER2:342_-C, [^111^In]-DOTA-H_6_-Z_HER2:342_-C, and [^111^In]-DOTA-Z_HER2:342_-H_6_-C). The attachment of ^125^I to the various Affibodies was performed with 1-[2-(4-hydroxyphenyl)ethyl]pyrrole-2,5-dione (HPEM; [^125^I]-HPEM-(HE)_3_-Z_HER2:342_-C, [^125^I]-HPEM-H_6_-Z_HER2:342_-C, and [^125^I]-HPEM-Z_HER2:342_-H_6_-C), and ^99m^Tc was coupled to the Affibody molecules with the N_3_S chelator formed between the thiol on the cysteine residue and the amide groups of the neighboring amino acids ([^99m^Tc]-(HE)_3_-Z_HER2:342_-C, [^99m^Tc]-H_6_-Z_HER2:342_-C, and [^99m^Tc]-(HE)_3_-Z_HER2:342_-C). The radiochemical yields (RCY) of the various ^111^In-labeled Affibody conjugates were >98.9 ± 0.2%. The RCY of the ^125^I conjugates ranged from 32.0 ± 1.0% to 36.2 ± 3.0%, and for the ^99m^Tc constructs the RCY ranged from 76.5 ± 1.0% to 99.3 ± 0.5%. Only the ^99m^Tc- and ^125^I-labeled Affibodies were purified further before use (12). The radiochemical purity of the final preparation of each radiolabeled Affibody was >98%. The specific activity and stability of the different radiolabeled Affibody constructs were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20affibody%20in%20vitro&cmd=DetailsSearch)]

The receptor binding specificity of [^111^In]-DOTA-, [^125^I]-HPEM-, and [^99m^Tc]-labeled (HE)_3_-Z_HER2:342_-C, H_6_-Z_HER2:342_-C, and Z_HER2:342_-H_6_-C was investigated by exposing SKOV-3 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology) to the different tracers in the presence or absence of 1,000-fold molar excess Z_HER2:342_ (12). Cellular binding of the different radiolabeled Affibodies ranged from 19.6 ± 1.0% ([^125^I]-HPEM-(HE)_3_-Z_HER2:342_-C) to 55.1 ± 0.4% ([^111^In]-DOTA-(HE)_3_-Z_HER2:342_-C) of the total added radioactivity. Binding of the labeled Affibodies to the blocked cells was significantly reduced (P < 0.0005) and ranged from 0.5 ± 0.0% ([^99m^Tc]-(HE)_3_-Z_HER2:342_-C) to 8.9 ± 0.8% ([^125^I]-HPEM-(HE)_3_-Z_HER2:342_-C) of the total added radioactivity. From this study, the investigators concluded that the labeled Affibodies had a high binding specificity for HER2 even though the various constructs had different chemistries (12). The affinity constants of the different Affibodies are presented in Table 1.

Table 1: Affinity constants for (HE) _ 3 _ -Z _ HER2:342 _ -C, H _ 6 _ -Z _ HER2:342 _ -C, and Z _ HER2:342 _ -H _ 6 _ -C

Constant | (HE) _ 3 _ -Z _ HER2:342 _ - C | H _ 6 _ -Z _ HER2:342 _ -C | Z _ HER2:342 _ -H _ 6 _ -C
Dissociation equilibrium constant, KD (pM) | 41 | 42 | 36
Association equilibrium constant, k _ a _ (M ^ -1 ^ s ^ -1 ^ ) | 5.8 × 10 ^ 6 ^ | 4.3 × 10 ^ 6 ^ | 1.2 × 10 ^ 7 ^
Dissociation equilibrium constant, k _ d _ (s ^ -1 ^ ) | 2.4 × 10 ^ -4 ^ | 1.8 × 10 ^ -4 ^ | 4.4 × 10 ^ -4 ^

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20affibody%20rodentia&cmd=DetailsSearch)]

The biodistribution of ^111^In-, ^125^I-, and ^99m^Tc-labeled Z_HER2:342_-C was studied in Naval Medical Research Institute mice as detailed by Hofstrom et al. (12). The animals (n = 4 mice/label per conjugate) were intravenously injected with 40 kBq (1.08 μCi, 0.71 nmol) of each radioactive conjugate and euthanized at 4 h postinjection. All organs of interest, including blood, were removed from the rodents, and the amount of label accumulated in the tissues was determined (Table 2). The uptake in each organ was expressed as a percent of injected activity per gram tissue (% IA/g). There was a low accumulation of label in the liver with all the radiolabeled Affibodies. Both the ^111^In- and ^99m^Tc-labeled Affibodies showed a high uptake in the kidneys, indicating that the radioactivity from these tracers was excreted primarily through the renal route. Compared with the ^111^In- and the ^99m^Tc-labeled Affibodies, a high accumulation of radioactivity was observed in the salivary gland (5.0% IA/g versus <1.0% IA/g), stomach (5.0% IA/g versus <1.0% IA/g), and the intestine (11.0% IA/g versus <1.5% IA/g) with [^125^I]-HPEM conjugates. The high accumulation of ^125^I in these organs was attributed to the intracellular retention of catabolites generated from the radioiodinated proteins. Among the [^111^In]-DOTA- and [^99m^Tc]-conjugates of the Affibodies, the (HE)_3_-Z_HER2:342_-C constructs showed the lowest accumulation of radioactivity in the liver.

Table 2: Biodistribution of [ ^ 111 ^ In]-DOTA-, [ ^ 125 ^ I]-HPEM-, and [ ^ 99m ^ Tc]-conjugates of (HE) _ 3 _ -Z _ HER2:342 _ -C, H _ 6 _ -Z _ HER2:342 _ -C, and Z _ HER2:342 _ -H _ 6 _ -C in select tissues of mice ( 12 ).

Organ* | Uptake of radioactivity (% IA/g, values are approximate)
Organ* | Label
Organ* | [ ^ 111 ^ In]-DOTA | | | [ ^ 125 ^ I]-HPEM | | | [ ^ 99m ^ Tc]
Organ* | Conjugate
Organ* | (HE) _ 3 _ -Z _ HER2:342 _ - C | H _ 6 _ -Z _ HER2:342 _ -C | Z _ HER2:342 _ -H _ 6 _ -C | (HE) _ 3 _ -Z _ HER2:342 _ - C | H _ 6 _ -Z _ HER2:342 _ -C | Z _ HER2:342 _ -H _ 6 _ -C | (HE) _ 3 _ -Z _ HER2:342 _ - C | H _ 6 _ -Z _ HER2:342 _ -C | Z _ HER2:342 _ -H _ 6 _ -C
Liver | 1.5 | 7.5 | 2.5 | 2.0 | 2.0 | 3.0 | <1.0 | 6.5 | 12.5
Kidney | 200.0 | 180.0 | 205.0 | 2.5 | 2.6 | 2.5 | 125 | 100.0 | 100.0
S. gland | <1.0 | <1.0 | <1.0 | 5.0 | 5.2 | 5.5 | <0.5 | <0.5 | <0.5
Stomach | <1.0 | <1.0 | <1.0 | 5.0 | 6.0 | 9.5 | <0.5 | <0.5 | <0.5
Intestine | 1.0 | 1.2 | 1.3 | 11.0 | 15.0 | 13.5 | 1.5 | 1.6 | 1.6
Whole carcass# | 2.5 | 2.7 | 4.0 | 10.0 | 8.5 | 9.0 | 1.5 | 1.7 | 2.0

*The uptake of radioactivity in the other organs (blood, lung, spleen, muscle, and bone) ranged from <0.5% IA/g to 2.5% IA/g; #, values expressed as % IA per whole sample.

From these studies, the investigators concluded that the (HE)_3_ tag was not only useful for purification of the Affibody, but it also improved the biodistribution profile of the molecule (reduced hepatic retention) in the rodents (12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20antibody%20non%20primate%20mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20antibody%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=her2%20antibody%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kramer-Marek G., Bernardo M., Kiesewetter D.O., Bagci U., Kuban M., Omer A., Zielinski R., Seidel J., Choyke P., Capala J. (2012). PET of HER2-Positive Pulmonary Metastases with 18F-ZHER2:342 Affibody in a Murine Model of Breast Cancer: Comparison with 18F-FDG. J Nucl Med.
2 Kramer-Marek G., Gijsen M., Kiesewetter D.O., Bennett R., Roxanis I., Zielinski R., Kong A., Capala J. (2012). Potential of PET to predict the response to trastuzumab treatment in an ErbB2-positive human xenograft tumor model. J Nucl Med.
3 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
4 Lofblom J., Feldwisch J., Tolmachev V., Carlsson J., Stahl S., Frejd F.Y. (2010). Affibody molecules: engineered proteins for therapeutic, diagnostic and biotechnological applications. FEBS Lett.
5 Tolmachev V., Orlova A. (2010). Influence of labelling methods on biodistribution and imaging properties of radiolabelled peptides for visualisation of molecular therapeutic targets. Curr Med Chem.
6 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
7 Ekblad T., Orlova A., Feldwisch J., Wennborg A., Karlstrom A.E., Tolmachev V. (2009). Positioning of 99mTc-chelators influences radiolabeling, stability and biodistribution of Affibody molecules. Bioorg Med Chem Lett.
8 Orlova A., Nilsson F.Y., Wikman M., Widstrom C., Stahl S., Carlsson J., Tolmachev V. (2006). Comparative in vivo evaluation of technetium and iodine labels on an anti-HER2 affibody for single-photon imaging of HER2 expression in tumors. J Nucl Med.
9 Ahlgren S., Wallberg H., Tran T.A., Widstrom C., Hjertman M., Abrahmsen L., Berndorff D., Dinkelborg L.M., Cyr J.E., Feldwisch J., Orlova A., Tolmachev V. (2009). Targeting of HER2-expressing tumors with a site-specifically 99mTc-labeled recombinant affibody molecule, ZHER2:2395, with C-terminally engineered cysteine. J Nucl Med.
10 Tolmachev V., Hofstrom C., Malmberg J., Ahlgren S., Hosseinimehr S.J., Sandstrom M., Abrahmsen L., Orlova A., Graslund T. (2010). HEHEHE-tagged affibody molecule may be purified by IMAC, is conveniently labeled with [(9)(9)(m)Tc(CO)(3)](+), and shows improved biodistribution with reduced hepatic radioactivity accumulation. Bioconjug Chem.
11 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
12 Hofstrom C., Orlova A., Altai M., Wangsell F., Graslund T., Tolmachev V. (2011). Use of a HEHEHE purification tag instead of a hexahistidine tag improves biodistribution of affibody molecules site-specifically labeled with (99m)Tc, (111)In, and (125)I. J Med Chem.